# [^111^In]-DOTA-Aminohexanoyl-[D-Phe^6^,Leu-NHCH_2_CH_2_CH_3_^13^,desMet^14^] BBN[6-14]

Chemical name: | [^111^In]-DOTA-Aminohexanoyl-[D-Phe^6^,Leu-NHCH_2_CH_2_CH_3_^13^,desMet^14^] BBN[6-14] | [image]
Abbreviated name: | [^111^In]Bomproamide; ^111^In-1 | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Gastrin-releasing peptide receptor (GRP-R) | [image]
Target Category: | Receptor | [image]
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^111^In]bompromide.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=gastrin%20releasing%20peptide%20receptor&cmd=DetailsSearch)]

The gastrin-releasing peptide (GPR), a bombesin (BBN) analog that targets the GRP receptor (GRP-R) to mediate its activity, is believed to assist in the progression and metastases of a variety of human cancers by acting as a growth factor (1, 2). Also, because the overexpression of GRP-R has been documented for many cancers, this receptor has been targeted with radiopharmaceuticals for the treatment of different malignancies, including that of the prostate (1). For a satisfactory therapeutic response with radiochemicals such as radiolabeled GRP, BBN, or their analogs, an optimal cellular accumulation of the radionuclide is necessary, and the uptake process is mediated by endocytosis, resulting in internalization of the receptor-ligand (RL) complex (3). Because the RL complex internalization is upregulated by the interaction of an agonist with its receptor, investigators in the field developed different radiolabeled BBN analogs that were GRP-R agonists and evaluated their biological characteristics under in vitro and in vivo conditions (3). Results obtained from several such studies showed that, in general, cellular uptake of the respective labeled agonists was low due to low affinity and binding to the receptor, and these compounds behaved more like antagonists rather than agonists (3). Compared to the agonists, compounds with antagonist activity are known to have a higher affinity for the receptor, can block the effects of an agonist, do not accelerate receptor internalization, and are now increasingly used for diagnostic purposes (3).

Many BBN analogs have been synthesized, and studies for their affinity to the GRP-R are described elsewhere (3). From these studies it was concluded that modifications at the C-terminus of BBN yielded compounds with agonistic properties that resulted in increased binding, but reduced internalization of the compound (3). Therefore, the C-terminal–modified BBN analogs were suitable for cancer diagnosis applications. Nock et al. developed a ^99m^Tc-labeled GRP-R antagonist, Demobesin 1, and investigated its biodistribution and use as an imaging agent for GRP-R–expressing tumors in nude mice (4) (Demobesin 1 is an N-terminal modified BBN analogue structurally based on a potent GRP-R antagonist; this agent has been discussed separately in MICAD, www.micad.nih.gov (5)). Although very low cellular internalization of [^99m^Tc]-Demobesin 1 was observed, it showed a high tumor accumulation with a long duration, suggesting that the labeled compound was suitable for diagnostic imaging. Similar results were also obtained with other ^99m^Tc-labeled N-terminal derivatives of BBN ([^99m^Tc]-Demobesin 3 and 4) as described elsewhere (6, 7). As an alternative to the existing compounds, another C-terminal–modified, ^111^In-labeled GRP-R antagonist BBN analog, [^111^In]-DOTA-aminohexanoyl-[D-Phe^6^,Leu-NHCH_2_CH_2_CH_3_^13^,desMet_14_] BBN[6-14] ([^111^In]bomproamide) was synthesized, and its biodistribution was studied in normal mice by Abd-Elgaliel et al. (3). The radiochemical was also evaluated for its imaging properties with single-photon emission tomography/computed tomography (SPECT/CT) in mice bearing tumors derived from PC-3 cells, which are of human prostate cancer origin and have a high level of GRP-R expression.

### Other sources of information

Other GRP-R chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Gastrin+releasing+peptide+receptor+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

GRP-R in Online Mendelian Inheritance in Man (OMIM) Database (http://www.ncbi.nlm.nih.gov/omim?term=Gastrin%20releasing%20peptide%20receptor)

Protein and mRNA sequence of human GRP-R (http://www.ncbi.nlm.nih.gov/nuccore/NM_005314.2)

Human GRP-R gene (GeneID: 2925) (http://www.ncbi.nlm.nih.gov/gene/2925)

Clinical trials on GRP-R (http://clinicaltrials.gov/ct2/results?term=gastrin+releasing+peptide+receptor)

US FDA information on GRP-R agonists (http://google2.fda.gov/search?q=Gastrin+releasing+peptide+receptor+agonist&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*)

US FDA information on GRP-R antagonists (http://google2.fda.gov/search?q=Gastrin+releasing+peptide+receptor+antagonists&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&sort=date%3AD%3AL%3Ad1&entqr=3&oe=UTF-8&ie=UTF-8&ud=1&site=FDAgov)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DBomproamide%20synthesis&cmd=DetailsSearch)]

The synthesis and ^111^In labeling of bomproamide has been described by Abd-Elgaliel et al. (3). The yield of the radiochemical was ~75–80% with a radiochemical purity of ≥99% as determined with high-performance liquid chromatography. The specific activity and stability of the labeled compound were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DBomproamide%20in%20vitro&cmd=DetailsSearch)]

In a competitive binding assay with ^125^I-Tyr^4^-BBN and PC-3 cells, bomproamide was shown to have an affinity of 1.36 ± 0.09 nM toward the GRP-R (3).

The cellular internalization of [^111^In]bomproamide was investigated by exposing PC-3 cells to the labeled compound under in vitro conditions (3). Internalization of the radiochemical was reported to plateau at ~14% of the added label after exposure for 45 min and remained constant up to 120 min. Subsequently, almost no label was lost from the cells for up to 90 min after internalization, indicating that loss (externalization) of radioactivity from the cells was extremely slow.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DBomproamide%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]bomproamide was investigated in normal CF-1 mice (3). The labeled compound was administered to the animals through the tail vein, and the mice were euthanized at predetermined time points (n = 5 mice/time point) ranging from 0.25 to 24 h postinjection (p.i.). All major organs were removed from the euthanized animals, and accumulated radioactivity in the various tissues was determined. Data were presented as percent of injected dose per gram tissue (% ID/g). At 0.25 h p.i., the pancreas exhibited the greatest radioactivity accumulation (12.21 ± 3.2% ID/g; among all the organs, the pancreas had the highest expression of GRP-Rs), followed by the kidneys (7.56 ± 0.89% ID/g) and blood (3.30 ± 2.98% ID/g). All other organs showed <2% ID/g of accumulated radioactivity. By 1 h p.i., the amount of radioactivity in the kidneys was reduced to 1.74 ± 0.32% ID/g, followed by the pancreas (0.95 ± 0.26% ID/g); all other tissues had <0.5% ID/g of the label at this time point. By 24 h p.i., all organs had negligible amounts of radioactivity (<0.1% ID/g). By 1 h p.i., 94.70 ± 0.62% of the radioactivity had been lost through the urinary route.

For blocking studies, CF-1 mice (n = 3 animals/group) were injected with [^111^In]bomproamide as before in presence or absence of unlabeled 100 μg BBN (3). Radioactivity accumulation in the main organs of the animals was determined at 1 h p.i. In general, animals injected with a blocking dose of BBN showed a reduced uptake of radioactivity compared to the controls; for example, accumulation in the pancreas of blocked animals was 0.20 ± 0.01% ID/g compared to 2.04 ± 0.17% ID/g in the control animals. From this study the investigators concluded that [^111^In]bomproamide had a high binding specificity for the GRP-R.

In another study, the biodistribution of [^111^In]bomproamide was studied in severe combined immune deficient (SCID) mice bearing a PC-3 cell tumor on each flank (3). The animals (n = 5 mice/time point) were euthanized at various time points ranging from 0.25 to 4 h p.i. Organs and tumors were harvested from the mice and used to determine the amount of radioactivity accumulated in the tissue. The pattern of radioactivity accumulation in the various tissues was similar to that obtained with the biodistribution studies described above. The tumors had 6.90 ± 1.06% ID/g label at 0.25 h, which gradually dropped to 2.15 ± 0.36% ID/g at 4 h p.i. The tumor/blood and tumor/muscle ratios were both 108.5 at 4 h p.i. No blocking studies were presented for the biodistribution study, although the pancreatic uptake of [^111^In]bomproamide was shown to be specific in CF-1 mice (see above).

MicroSPECT/CT imaging was performed on a single SCID mouse bearing PC-3 cell xenograft tumors as described by Abd-Elgaliel et al. (3). Imaging was initiated at 1 h p.i. and performed over 16 h. The PC-3 xenograft tumors and the kidneys were clearly visible in the images, and the imaging data were consistent with biodistribution of the labeled compound described above. No blocking studies were presented.

With results obtained from these studies, the investigators concluded that C-terminal–modified BBN analogs can be used for the diagnostic imaging of tumors overexpressing the GRP-R (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dbomproamide%20non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dbomproamide%20non-human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dbomproamide%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

National Cancer Institute grant P50 CA 103130

## References

1 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
2 Cornelio D.B., Roesler R., Schwartsmann G. (2007). Gastrin-releasing peptide receptor as a molecular target in experimental anticancer therapy. Ann Oncol.
3 Abd-Elgaliel W.R., Gallazzi F., Garrison J.C., Rold T.L., Sieckman G.L., Figueroa S.D., Hoffman T.J., Lever S.Z. (2008). Design, synthesis, and biological evaluation of an antagonist-bombesin analogue as targeting vector. Bioconjug Chem.
4 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
5 Shan, L., [99mTc-N40-1-bzlg0,D-Phe6,Leu-NHEt13,des-Met14]Bombesin(6–14). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
6 Nock B.A., Nikolopoulou A., Galanis A., Cordopatis P., Waser B., Reubi J.C., Maina T. (2005). Potent bombesin-like peptides for GRP-receptor targeting of tumors with 99mTc: a preclinical study. J Med Chem.
7 Shan, L., 99mTc-labeled [N40,Pro1,Tyr4]bombesin. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.